# Cy5.5-Rituximab

Chemical name: | Cy5.5-Rituximab
Abbreviated name: | Cy5.5-RIT
Synonym: | Cy5.5-Rituxan®
Agent category: | Antibody
Target: | CD20
Target category: | Antigen
Method of detection: | Optical, near-infrared (NIR) fluorescence
Source of signal: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=309156), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=224994198) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=931) for more information about CD20.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cy5.5+Rituximab)]

Optical fluorescence imaging is increasingly used to obtain biological functions of specific targets in small animals (1, 2). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging.

CD20 is a nonglycosylated phosphoprotein specific for the B-cell lymphocytes, and it plays an important role in B-cell development (3). Its expression is absent in the pro-B-cells and plasma B-cells, the first stage and the last stage of B-cell differentiation, respectively. CD20 is expressed on the cell surface of B-cell lymphoma, hairy cell leukemia, and B-cell chronic lymphocytic leukemia (4). Rituximab (RIT), a humanized monoclonal antibody (mAb) directed toward CD20, is approved by the United States Food and Drug Administration to treat B-cell lymphoma and leukemia (5). It is also under investigation in several clinical trials (http://clinicaltrials.gov/ct2/results?term=rituximab) for combination treatments with chemotherapy (6). RIT has been conjugated with Cy5.5 (Cy5.5-RIT) to study in vivo biodistribution of Cy5.5-RIT in tumor-bearing mice (7). Cy5.5-RIT has been found to have a good accumulation in lymphoma tumor cells in nude mice. Cy5.5 is a NIR fluorescence dye with an absorbance maximum at 675 nm and an emission maximum at 694 nm, with a high extinction coefficient of 250,000 M^-1^cm^-1^.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cy5.5+Rituximab+synthesis)]

RIT (6.6 nmol) was conjugated with Cy5.5-N-hydroxysuccinimide (NHS) ester (0.05 mg) to form Cy5.5-RIT after incubation for 1 h at room temperature (7). The NHS ester of Cy5.5 reacted with the ε-amino group of the lysine moieties of RIT. Cy5.5-RIT was purified with dialysis. There were three Cy5.5 dye molecules per RIT molecule. The labeling yield was 46%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cy5.5+Rituximab+and+in+vitro)]

Biffi et al. (7) performed flow cytometric analysis with Cy5.5-RIT and RIT using the CD20-expressing human BJAB lymphoma cell line. Binding of Cy5.5-RIT and unlabeled RIT to the BJAB cells were similar, indicating that the immunoreactivity of Cy5.5-RIT was similar to the parent mAb. Control FITC-IgG_1_ was not able to bind the BJAB cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cy5.5+Rituximab+rodentia)]

Biffi et al. (7) performed whole-body NIR fluorescence imaging studies of Cy5.5-RIT in nude mice bearing subcutaneous BJAB lymphoma xenografts. Images were obtained after intravenous injection of 1 nmol of the tracer. Substantial contrasts were observed between the BJAB tumor and normal tissue from ~4 h with a maximal difference at 48 h. The NIR fluorescence intensity of the tumor slowly decreased over the following 8 days. The liver showed the fastest initial accumulation of the probe with gradual washout. Ex vivo imaging showed that most of the Cy5.5-RIT NIR fluorescence intensity was found in the tumor, with the liver exhibiting the second highest signal intensity; low signal intensities were observed in the kidneys, heart, lung, and spleen. Immunohistochemical staining showed that strong membrane binding to anti-CD20 antibody in the tumor was colocalized with RIT binding in the periphery of the primary tumor. However, no blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cy5.5+Rituximab+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cy5.5+Rituximab+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cy5.5+Rituximab+human)]

No publication is currently available.

## References

1 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
2 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
3 Reff M.E., Carner K., Chambers K.S., Chinn P.C., Leonard J.E., Raab R., Newman R.A., Hanna N., Anderson D.R. (1994). Depletion of B cells in vivo by a chimeric mouse human monoclonal antibody to CD20. Blood.
4 McLaughlin, P., C.A. White, A.J. Grillo-Lopez, and D.G. Maloney, Clinical status and optimal use of rituximab for B-cell lymphomas. Oncology (Williston Park), 199812(12): p. 1763-9; discussion 1769-70, 1775-7.
5 Cheson B.D. (2006). Monoclonal antibody therapy for B-cell malignancies. Semin Oncol.
6 Tsirigotis P., Economopoulos T. (2008). Monoclonal antibodies in the treatment of lymphoid malignancies. J Steroid Biochem Mol Biol.
7 Biffi S., Garrovo C., Macor P., Tripodo C., Zorzet S., Secco E., Tedesco F., Lorusso V. (2008). In vivo biodistribution and lifetime analysis of cy5.5-conjugated rituximab in mice bearing lymphoid tumor xenograft using time-domain near-infrared optical imaging. Mol Imaging.